# ^125^I-Single-chain antibody B5 targeting a pancreatic β-cell surface antigen

Chemical name: | ^125^I-Single-chain antibody B5 targeting a pancreatic β-cell surface antigen
Abbreviated name: | ^125^I-SCA B5
Synonym:
Agent category: | Antibody
Target: | Pancreatic β-cell specific antigen
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5)]

The β-cell mass (BCM) is a useful indicator of the function of the pancreas. In type I diabetes, β-cells are destroyed, leading to a dramatic decrease in BCM. In type II diabetes, there is a slow and continuous decrease in BCM because of peripheral insulin resistance and increased demand for insulin. Vesicular monoamine transporter (VMAT2) is present in brain monoaminergic neurons and is responsible for collecting neurotransmitters (e.g., dopamine, norepinephrine, and serotonin) from the cytoplasm and storing them in vesicles for synaptic release (1). VMAT2 is also highly expressed by β-cells in the endocrine pancreas but not in the exocrine pancreas. VMAT2 is expressed mainly on the β-cells in the islets of Langerhans and comprises 1%–2% of the pancreatic mass. VMAT2 is a potential target for noninvasive assessment of BCM and pancreatic function. VMAT2 has been studied noninvasively in vivo with positron emission tomography (PET) using [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine, also known as [^11^C]DTBZ (http://www.ncbi.nlm.nih.gov/books/NBK23597/)) in the human brain and pancreas. However, a human clinical study showed that the high nonspecific binding in the exocrine pancreas may appear to overestimate BCM on pancreatic [^11^C]DTBZ PET scans (2). Glucagon-like peptide-1 receptor (GLP-1R) has been shown to be highly overexpressed in human insulinomas and gastrinomas and has been evaluated with various noninvasive imaging studies of β-cells (3-5). Other β-cell imaging probes have also been studied (6-8).

Brogren et al. (9) prepared a rat monoclonal autoantibody (IC2) with lymphocytes isolated from the spleen and lymph nodes of a spontaneously diabetic BB rat. IC2 is a rat IgM kappa monoclonal antibody. The binding of IC2 to β-cells is sensitive to protease treatments. IC2 shows little binding to other rat tissues; however, IC2 exhibits binding to mouse, hamster, and human β-cells (8). Moore et al. (10) showed ^111^In-diethylenetriamine pentaacetic acid-IC2 (^111^In-DTPA-IC2 (http://www.ncbi.nlm.nih.gov/books/NBK83903/)) binding to β-cells in normal mice and reduced binding to β-cells in mice treated with streptozotocin (STZ) to induce BCM loss and diabetes. However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (11). Smaller antibody fragments, such as single-chain antibody (SCA), Fab' or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys (12). SCA comprises a single polypeptide in which the V_H_ (variable heavy chain) and V_L_ (variable light chain) domains are attached to one another by a flexible linker. Using phage-display screening of human SCA library with a rat β-cell insulinoma INS-1 tumor cell line, Ueberberg et al. (13) identified SCA B5 to be β-cell-specific. ^125^I-SCA B5 has been evaluated as a potential imaging probe for β-cells.

### Related Resource Links:

- Chapters in MICAD (β-cells (http://www.ncbi.nlm.nih.gov/books?term=beta-cell%20AND%20micad%5Bbook%5D), GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (VMAT2 (http://www.ncbi.nlm.nih.gov/gene/6571), GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VMAT2 (http://www.ncbi.nlm.nih.gov/omim/193001), GLP-1R (http://omim.org/entry/138032))
- Clinical trials (VMAT2 (http://www.clinicaltrials.gov/ct2/results?term=VMAT2), Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (VMAT2 (http://google2.fda.gov/search?q=VMAT2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=10), Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+synthesis)]

SCA B5 were labeled with ^125^I using the chloramine-T method as described previously (14). The radiochemical purity, specific activity, and labeling yield of ^125^I-SCA B5 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+in+vitro)]

Ueberberg et al. (13) performed in vitro indirect fluorescence staining with SCA B5 on rat insulinoma INS-1 cells (pancreatic β-cells) and rat AR42J pancreatic exocrine tumor cells (control) at 4ºC. Confocal microscopy showed strong fluorescence signal on the cell surface of INS-1 cells but weak or no signal in AR42J cells. INS-1 cells exhibited 450-fold higher fluorescence intensity than AR42J cells. Fluorescence signal was detected in the cytoplasm of INS-1 cells incubated with SCA B5 for 10 min at 37ºC, indicating SCA internalization. ^125^I-SCA B5 showed rapid binding to INS-1 cells, with a binding half-life of 6 min and no washout, suggesting internalization of ^125^I-SCA B5. No blocking studies were carried out. The ^125^I-SCA B5 binding at 4ºC was saturable with a binding constant (K_d_) of 3.6 µM and 858 binding sites/cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+rodentia)]

Ex vivo biodistribution studies were performed in non-diabetic CD mice (n = 6) at 2 h after injection of 18.5 MBq (0.5 mCi (2.5 nmol)) ^125^I-SCA B5 (13). The organ with the highest uptake was the pancreas (5.12 ± 1.01% injected dose/g (ID/g)), followed by the liver (0.71 ± 0.28% ID/g), stomach (0.69 ± 0.24% ID/g), spleen (0.55 ± 018% ID/g), kidneys (0.38 ± 0.13% ID/g), thyroid (0.27 ± 15% ID/g), brain (0.26 ± 0.09% ID/g), and blood (0.23 ± 0.11% ID/g). Pretreatment with unlabeled SCA B5 (2.5 nmol) 15 min before ^125^I-SCA B5 injection significantly reduced the radioactivity in the pancreas to 0.95 ± 0.18% ID/g (P < 0.001), with little inhibition in the other organs. Histoimmunostaining showed a co-localization of SCA B5 to the insulin-positive β-cells in the pancreatic islets with no binding to the glucagon-producing exocrine cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SCA%20B5+human)]

No publication is currently available.

## NIH support

DK072473

## References

1 Schuldiner S. (1994). A molecular glimpse of vesicular monoamine transporters. J Neurochem.
2 Goland R., Freeby M., Parsey R., Saisho Y., Kumar D., Simpson N., Hirsch J., Prince M., Maffei A., Mann J.J., Butler P.C., Van Heertum R., Leibel R.L., Ichise M., Harris P.E. (2009). 11C-dihydrotetrabenazine PET of the pancreas in subjects with long-standing type 1 diabetes and in healthy controls. J Nucl Med.
3 Brom M., Oyen W.J., Joosten L., Gotthardt M., Boerman O.C. (2010). 68Ga-labelled exendin-3, a new agent for the detection of insulinomas with PET. Eur J Nucl Med Mol Imaging.
4 Christ E., Wild D., Forrer F., Brandle M., Sahli R., Clerici T., Gloor B., Martius F., Maecke H., Reubi J.C. (2009). Glucagon-like peptide-1 receptor imaging for localization of insulinomas. J Clin Endocrinol Metab.
5 Reiner T., Thurber G., Gaglia J., Vinegoni C., Liew C.W., Upadhyay R., Kohler R.H., Li L., Kulkarni R.N., Benoist C., Mathis D., Weissleder R. (2011). Accurate measurement of pancreatic islet beta-cell mass using a second-generation fluorescent exendin-4 analog. Proc Natl Acad Sci U S A.
6 Malaisse W.J., Louchami K., Sener A. (2009). Noninvasive imaging of pancreatic beta cells. Nat Rev Endocrinol.
7 Moore A. (2009). Advances in beta-cell imaging. Eur J Radiol.
8 Saudek F., Brogren C.H., Manohar S. (2008). Imaging the Beta-cell mass: why and how. Rev Diabet Stud.
9 Brogren C.H., Hirsch F., Wood P., Druet P., Poussier P. (1986). Production and characterization of a monoclonal islet cell surface autoantibody from the BB rat. Diabetologia.
10 Moore A., Bonner-Weir S., Weissleder R. (2001). Noninvasive in vivo measurement of beta-cell mass in mouse model of diabetes. Diabetes.
11 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
12 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
13 Ueberberg S., Ziegler D., Schechinger W., Dietrich J.W., Akinturk S., Klein H.H., Schneider S. (2010). In vitro phage display in a rat beta cell line: a simple approach for the generation of a single-chain antibody targeting a novel beta cell-specific epitope. Diabetologia.
14 Hampe C.S., Wallen A.R., Schlosser M., Ziegler M., Sweet I.R. (2005). Quantitative evaluation of a monoclonal antibody and its fragment as potential markers for pancreatic beta cell mass. Exp Clin Endocrinol Diabetes.